# Methyl 2-(2-[^18^F]fluoro-4-nitrobenzamido)-3- methylbutanoic acid

Chemical name: | Methyl 2-(2-[^18^F]fluoro-4-nitrobenzamido)-3- methylbutanoic acid
Abbreviated name: | [^18^F]FNBMBA
Synonym: | [^18^F]1; (2S)-2-[(4-amino-2-fluoranylbenzoyl)amino]-3-methylbutanoic acid
Agent Category: | Compound
Target: | Tumors
Target Category: | Nonspecific tissues
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | [^18^F]
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^18^F]FNBMBA for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB)]

The most commonly used radiochemical for positron emission tomography (PET) imaging of brain or systemic cancerous tumors is 2-[^18^F]fluorodeoxyglucose ([^18^F]FDG), a radiotracer approved by the United States Food and Drug Administration for imaging purposes, but the use of this radiolabel is not without limitations because, among several application drawbacks, it tends to produce a high background in the brain and inflamed tissues during imaging (1, 2). To circumvent problems encountered with [^18^F]FDG, some investigators developed and evaluated unnatural amino acid (aa) derivatives such as O-2-[^18^F]fluoroethyl-L-tyrosine (L-[^18^F]FET) for the detection of tumors, particularly of the brain, and it was shown that L-[^18^F]FET was superior to [^18^F]FDG in distinguishing tumors from inflammation (3). However, the synthesis of ^18^F-labeled aa is cumbersome and, because an electrophilic substitution reaction is used to introduce the label into the aa, the final labeled product yields are very low (2). An alternative synthetic method of placing a fluoroalkyl group on the aromatic ring of tyrosine was observed to improve the yield of L-[^18^F]FET, but it prolonged the synthesis time for the radiochemical (4, 5). In an effort to simplify the synthesis of ^18^F-radiolabeled aas, ^18^F-labeled fluoroarylvaline derivatives of L-valine were prepared after modifying the aa with 2,4-dinitrobenzoic acid (2). According to the investigators, introduction of ^18^F at the ortho-position of 2,4-dinitrobenzoic acid is very easy, and the attachment of this moiety to L-valine results in an improved lipophilicity of the molecule. Using this method, two derivatives of L-valine were produced: methyl 2-(2-[^18^F]fluoro-4-nitrobenzamido)-3-methylbutanoate ([^18^F]MFNBMB; [^18^F]1) and methyl 2-(2-[^18^F]fluoro-4-nitrobenzamido)-3-methylbutanoic acid ([^18^F]FNBMBA; [^18^F]2) (2). These radiotracers were evaluated under in vivo conditions, and their biological properties were compared with those of [^18^F]FDG and L-[^18^F]FET. This chapter describes the characteristics of [^18^F]FNBMBA and its biodistribution in tumor-bearing mice. The characteristics of [^18^F]MFNBMB and its biodistribution in tumor-bearing mice is described in a separate chapter of MICAD (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+synthesis)]

The synthesis of FNBMBA, with a yield of 66%, was detailed by Qiao et al. (2). Radiolabeling of FNBMBA to obtain [^18^F]FNBMBA was performed using a nucleophilic substitution denitrofluorination reaction as described elsewhere (2). The radiochemical yield of the synthesis was ~30–40% without decay correction, with chemical and radiochemical purity of >99%, respectively. The time required for the synthesis was ~100 min. The specific activity of the labeled compound was not reported.

[^18^F]FNBMBA was reported to be 100% stable, as determined with thin-layer chromatography and high-performance liquid chromatography (HPLC) in normal saline, phosphate-buffered saline (pH not reported), or 96% ethanol for up to 6 h at room temperature, and in ethanol, dimethylformamide, and acetonitrile for up to 30 min at 60°C (2). HPLC analysis of blood obtained from mice 30 min after treatment with [^18^F]FNBMBA showed that the radiolabeled compound was also stable under in vivo conditions.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+rodentia)]

The biodistribution of [^18^F]FNBMBA was investigated in mice bearing mouse sarcoma S180 cell tumors (2). The mice were injected with the radiolabeled compound through the tail vein, and the animals were euthanized at 5, 15, 30, 60, and 120 min (n = 4 animals/time point) after treatment. The tumor and other organs of interest were removed from the animals, and accumulated radioactivity was measured with a gamma counter (represented as percent of injected dose/gram tissue (% ID/g)). A rapid distribution of radioactivity in the various organs and tissue, within 5 min of injection, was observed. In general, by 120 min after the treatment a decrease in accumulated radioactivity was reported in all organs and tissue, including tumors. The tumor/blood ratio increased from 0.56 at 5 min to 2.32 at 30 min, and then decreased to 1.30 at 120 min. The tumor/brain ratio increased from 9.38 at 5 min to 13.30 at 30 min, and then decreased to 6.90 at 120 min. A similar trend was also noticed for the tumor/muscle ratio of the animals. The tumor/blood, tumor/brain, and tumor/muscle ratios with [^18^F]MFNBMB were lower than those obtained with [^18^F]FNBMBA (for comparison, see the MICAD chapter regarding [^18^F]MFNBMB (6)).

For comparison, a similar biodistribution study was also performed with the tumor-bearing mice using [^18^F]FDG and L-[^18^F]FET, respectively (2). The blood clearance of both [^18^F]FNBMBA and [^18^F]BFNBMB were reported to be slower than that of [^18^F]FDG, but faster than that of L-[^18^F]FET. Compared with [^18^F]FNBMBA, [^18^F]MFNBMB, or L-[^18^F]FET, the tumor/blood ratio for [^18^F]FDG increased from 1.17 at 5 min to 15.85 at 120 min. However, the tumor/brain ratio of [^18^F]FDG was much lower at all time points (from 0.53 at 5 min to 1.33 at 120 min) than that of the other three labeled compounds (9.38 at 5 min to 6.90 at 120 min for [^18^F]FNBMBA, 2.79 at 5 min to 2.61 at 120 min for [^18^F]MFNBMB, and 2.10 at 5 min to 2.95 at 120 min for L-[^18^F]FET). The tumor/muscle ratios of [^18^F]FDG and L-[^18^F]FET (0.81 and 0.72, respectively, at 5 min after injection) increased up to 120 min (2.20 for [^18^F]FDG and 1.40 for L-[^18^F]FET). In comparison, the ratios for [^18^F]MFNBMB and [^18^F]FNBMBA decreased from 1.94 and 1.38, respectively, at 5 min to 0.54 and 0.66, respectively, at 120 min.

From these studies, the investigators concluded that [^18^F]FNBMBA was superior to [^18^F]MFNBMB, [^18^F]FDG, and L-[^18^F]FET for the detection of brain tumors in mice (2). However, no studies were reported to investigate if the metabolic pathway followed by [^18^F]FNBMBA was the same as valine, its parent compound.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=MFNBMB+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Dunphy M.P., Lewis J.S. (2009). Radiopharmaceuticals in preclinical and clinical development for monitoring of therapy with PET. J Nucl Med.
2 Qiao Y., He Y., Zhang S., Li G., Liu H., Xu J., Wang X., Qi C., Peng C. (2009). Synthesis and evaluation of novel F-18 labeled fluoroarylvaline derivatives: potential PET imaging agents for tumor detection. Bioorg Med Chem Lett.
3 Lee T.S., Ahn S.H., Moon B.S., Chun K.S., Kang J.H., Cheon G.J., Choi C.W., Lim S.M. (2009). Comparison of 18F-FDG, 18F-FET and 18F-FLT for differentiation between tumor and inflammation in rats. Nucl Med Biol.
4 Heiss P., Mayer S., Herz M., Wester H.J., Schwaiger M., Senekowitsch-Schmidtke R. (1999). Investigation of transport mechanism and uptake kinetics of O-(2-[18F]fluoroethyl)-L-tyrosine in vitro and in vivo. J Nucl Med.
5 Wester H.J., Herz M., Weber W., Heiss P., Senekowitsch-Schmidtke R., Schwaiger M., Stocklin G. (1999). Synthesis and radiopharmacology of O-(2-[18F]fluoroethyl)-L-tyrosine for tumor imaging. J Nucl Med.
6 Chopra, A., Methyl 2-(2-[18F]fluoro-4-nitrobenzamido)-3-methylbutanoate. [[18F]MFNBMB]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.